# 4-[^18^F]Fluorobenzenecarbohydrazide-methotrexate

Chemical name: | 4-[^18^F]Fluorobenzenecarbohydrazide-methotrexate
Abbreviated name: | [^18^F]-Folate-MTX-8
Synonym: | [^18^F]-8
Agent Category: | Compound
Target: | Folate receptor
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on above structure for information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=folate%20receptor%20imaging&cmd=DetailsSearch)]

Folic acid (FA; also known as folate or vitamin B_9_) is a water-soluble vitamin that is required for the synthesis and repair of cellular DNA. FA also acts as a cofactor for many biological reactions and has an important role in cell maintenance and proliferation. Although the folate receptor (FR) is expressed at low levels in normal cells, this receptor is known to be upregulated in cancers such as those of the ovary, lung, breast, brain, colon, and the hematopoietic lineage cells (1). Therefore, the FR system has been targeted with radiolabeled folate and its derivatives, such as ^67^Ga-deferoxamine (DF)-folate, ^111^In-diethylenetriamine pentaacetic acid-folate, ^99m^Tc-mercaptoacetyldiglycine-folate-methotrexate, etc., for the noninvasive detection of malignancies with single-photon emission computed tomography (2). Mathias et al. showed that ^66/67^Ga-DF-folate can be used with positron emission tomography (PET) for the imaging of FR-positive cancerous tumors in mice (3). However, although these tracers could detect the FR-rich tumors, they were deemed unsuitable for imaging lesions in the abdominal regions because high levels of radioactivity were observed to accumulate in the liver and intestines of the animals (4). In addition, ^66/67^Ga-labeled tracers are known to produce low-resolution images because they generate high positron energy (4.15 MeV and 1.89 MeV for ^66^Ga and ^67^Ga, respectively. ^67^Ga-labeled agents are used for single photon emission computed tomography imaging) compared to ^18^F (0.64 MeV), which generates superior images and is often used to radiolabel PET imaging agents in the clinic (4). In another study, it was shown that ^18^F-fluorobenzylamine derivatives of folate could detect tumors that had a high expression of FR, but the radioactivity from these labeled compounds accumulated mainly at the rim of the tumor, and large amounts of the label were retained in the liver and intestines of the animals (4, 5).

In an ongoing effort to generate radiolabeled agents for the imaging of tumors that express high levels of FRs that would be superior to those developed and evaluated earlier, a ^18^F-fluorobenzene derivative of folic acid ([^18^F]-folate-1), a pyridinecarbohydrazide-folate derivative of folic acid ([^18^F]-folate-2), a ^18^F-fluorobenzene/methotrexate (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=78794e3d-f293-4eeb-22ac-8f536d5947eb) (MTX) conjugate of folic acid ([^18^F]-folate-MTX-8), and a ^18^F-pyridinecarbohydrazide-folate/methotrexate conjugate of folic acid ([^18^F]-folate-MTX-9) have been synthesized (2). The biodistribution of these tracers was investigated in healthy mice. On the basis of results obtained from these studies, [^18^F]-folate-2 was evaluated for the PET imaging of human KB cell line (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-17&Template=cellBiology) xenograft tumors (have a high expression of FR) in mice. This chapter describes the results obtained with [^18^F]-folate-MTX-8. Separate chapters in MICAD (www.micad.nih.gov) discuss the studies performed with [^18^F]-folate-1 (6), [^18^F]-folate-2 (7), and [^18^F]-folate-MTX-9 (8).

### Related Resource Links

FR-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Folate+receptor+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Adult human FR protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_016724.2)

Human FR gene (http://www.ncbi.nlm.nih.gov/gene/2348) (Gene ID: 2348)

FR clinical trials (http://clinicaltrials.gov/ct2/results?term=folate+receptor+AND+targeted+AND+cancer)

FR in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/136430) database

FR pathway in Kyoto Encyclopedia of Genes and Genomes (KEGG) (http://www.genome.jp/dbget-bin/www_bget?hsa:2348+hsa:2350+hsa:2352+hsa:390243)

Folic acid information on Dailymed site (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=ff80ef4d-e04c-9f83-2b56-cccc30028f72)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20synthesis&cmd=DetailsSearch)]

Folate-MTX-8 was obtained by the conjugation of the γ-isomer of N-succinimidyl-methotrexate carboxylate with 4-fluorobenzenecarbohydrazide in presence of triethylamine and labeled the resulting product with ^18^F as described by al Jammaz et al. (2). The synthesis and labeling of [^18^F]-folate-2 and [^18^F]-folate-1 have been detailed elsewhere (9). The total time of synthesis for each of the tracers was ~45 min, and the radiochemical yield and radiochemical purity of the final labeled products were >80% (based on the initial ^18^F concentration) and >97% (without high-performance liquid chromatographic purification), respectively. The specific activity of the different radiolabeled compounds was reported to be >11.11 MBq/μmol (300 mCi/μmol) (2).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20in%20vitro&cmd=DetailsSearch)]

Using an n-octanol-water mixture (pH 7.3), the partition coefficient of [^18^F]-folate-MTX-8 was determined to be 0.43. The partition coefficients of [^18^F]-folate-1 and [^18^F]-folate-2 were reported to be 0.38 ± 0.02 and 0.14 ± 0.01, respectively, indicating that these labeled compounds had a low lipophilicity and that, among the three tracers, [^18^F]-folate-2 was least lipophilic (9).

[^18^F]-Folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 were reported to be stable in human plasma for at least 4 h at 37°C (data not presented) (2).

From a saturation assay with KB cell membranes, the FR binding affinities of [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 were determined to be 22.52 ± 1.79 nM, 13.08 ± 0.83 nM, and 15.51 ± 1.80 nM, respectively (9). A cell internalization assay of [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 with KB cells (using an acidic buffer, pH not mentioned) showed that 23.42 ± 1.53%, 25.85 ± 0.95%, and 11.86 ± 0.43% of the tracers were respectively internalized by the cells within 20 min at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 was studied in normal Balb/c mice as described by Jammaz et al. (2). The animals (n = 4 mice/time point for each tracer) were injected with 749 kBq (20 μCi) of the tracer through the tail vein and euthanized at 10, 60, and 120 min postinjection (p.i.) to determine the amount of radioactivity accumulated in the various organs. All data were presented as percent of injected dose per gram tissue (% ID/g). The label from [^18^F]-folate-MTX-8 was cleared rapidly from the blood (5.64 ± 0.95% ID/g at 10 min p.i., 1.90 ± 0.28% ID/g at 60 min p.i., and 1.08 ± 0.25% ID/g at 120 min p.i.). The kidneys accumulated high levels of radioactivity (8.93 ± 1.49% ID/g at 10 min p.i. and 6.40 ± 1.35% ID/g at 120 min p.i.), and a similar trend was noted with the intestine (6.33 ± 0.19% ID/g at 10 min p.i. and 7.17 ± 1.56% ID/g at 120 min p.i.). This indicated that the tracer was excreted through the urinary and the hepatobiliary routes in the animals. With [^18^F]-folate-1, rapid clearance of radioactivity from the blood was observed (4.41 ± 0.60% ID/g at 10 min p.i., 2.55 ± 1.50% ID/g at 60 min p.i., and 1.13 ± 0.51% ID/g at 120 min p.i.). High levels of label from [^18^F]-folate-1 were observed in the kidneys (22.50 ± 4.42% ID/g at 10 min p.i. and 17.88% ID/g ± 0.10 at 120 min p.i.) and the intestine (5.95 ± 2.11% ID/g at 10 min p.i. and 5.86 ± 0.26% ID/g at 120 min p.i.) of these animals, indicating that this tracer also was excreted through the urinary and the hepatobiliary route. Radioactivity from [^18^F]-folate-2 was rapidly cleared from circulation (1.22 ± 0.61% ID/g at 10 min p.i., 0.10 ± 0.05% ID/g at 60 min p.i., and 0.04 ± 0.01% ID/g at 120 min p.i.). A high accumulation of label from [^18^F]-folate-2 was observed in the kidneys (13.8 ± 5.9% ID/g at 10 min p.i. and 2.92 ± 0.51% ID/g at 120 min p.i.), but the intestines accumulated a low level of the tracer (0.76 ± 0.20% ID/g at 10 min p.i. and 0.03 ± 0.01% ID/g at 120 min p.i.). This indicated that radioactivity from [^18^F]-folate-2 was excreted primarily through the urinary route. The accumulation of low levels of radioactivity with [^18^F]-folate-2 in the various organs suggested that this tracer had a superior pharmacokinetic profile compared to [^18^F]-folate-MTX-8 and [^18^F]-folate-1. No blocking studies with [^18^F]-folate-MTX-8 were reported.

The biodistribution of [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 was also investigated in nude mice (n = 4 animals/tracer) bearing KB cell tumors (2). The animals were injected with the radiotracers as described above and euthanized at 60 min p.i. With all the radiolabeled compounds, the uptake of radioactivity in the various organs of the mice at 60 min p.i. was similar to that observed earlier (see above). The tumor uptake of label with [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 at 60 min p.i. was 0.81 ± 0.09% ID/g, 5.94 ± 1.16% ID/g, and 5.74 ± 0.16% ID/g, respectively, indicating that the tumor uptake of radioactivity with [^18^F]-folate-MTX-8 was significantly lower (P < 0.05) than that observed with either [^18^F]-folate-1 or [^18^F]-folate-2. The tumor/blood and tumor/muscle ratios with [^18^F]-folate-MTX-8, [^18^F]-folate-1, and [^18^F]-folate-2 at 60 min p.i. were 0.80 and 1.63, 14.70 and 28.70, and 6.39 and 25.83, respectively. For blocking studies, the mice were injected with 100 μg (0.22 μmol) FA 10 min before the administration of [^18^F]-folate-MTX-8, [^18^F]-folate-1, or [^18^F]-folate-2, and the rodents were subsequently treated as before (2). With [^18^F]-folate-MTX-8, the tumors showed a significantly reduced (P < 0.05) uptake of radioactivity (0.19 ± 0.10% ID/g) at 60 min p.i., and a similar trend was evident in the kidneys, intestines, and liver (among these organs the kidney and the liver show a higher expression of FR compared with the other normal tissues). The tumors showed a significantly reduced accumulation of radioactivity (0.74 ± 0.17% ID/g, P < 0.05) with [^18^F]-folate-1 at 60 min p.i., and the kidneys, liver, and the intestines of the animals also showed a reduced level of the label (P < 0.05). With [^18^F]-folate-2, the uptake of radioactivity in the tumor at 60 min p.i. was reduced to 0.66 ± 0.10% ID/g (P < 0.05), and a similar trend was observed in the kidneys, liver, and intestines (P < 0.05). These studies indicated that only [^18^F]-folate-1 and [^18^F]-folate-2 had a high binding specificity for the FR in the tumors and the various organs of the animals.

Table: Tumor Uptake and Tumor/Blood and Tumor/Muscle Ratios of different ^ 18 ^ F-Labeled Folate and Folate-MXT Compounds

Tracer | Tumor Uptake (% ID/g) | | Ratio (No Folate Pre-treatment)
Tracer | No Folate Pre-treatment | With Folate (100 μg) Pre-treatment | Tumor/blood | Tumor/Muscle
[ ^ 18 ^ F]-Folate-1 | 5.94 ± 1.16 | 0.74 ± 0.17 | 6.39 | 25.83
[ ^ 18 ^ F]-Folate-2 | 5.74 ± 0.16 | 0.66 ± 0.10 | 14.72 | 28.70
[ ^ 18 ^ F]-Folate-MXT-8 | 0.18 ± 0.09 | 0.19 ± 0.10 | 0.90 | 1.80

From the studies and the results discussed above, the investigators concluded that [^18^F]-folate-2 was probably superior to either [^18^F]-folate-MTX-8 or [^18^F]-folate-1 for the imaging of FR-expressing tumors in rodents (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-F-1%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Xia W., Low P.S. (2010). Folate-targeted therapies for cancer. J Med Chem.
2 Al Jammaz I., Al-Otaibi B., Amer S., Okarvi S.M. (2011). Rapid synthesis and in vitro and in vivo evaluation of folic acid derivatives labeled with fluorine-18 for PET imaging of folate receptor-positive tumors. Nucl Med Biol.
3 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
4 Sega E.I., Low P.S. (2008). Tumor detection using folate receptor-targeted imaging agents. Cancer Metastasis Rev.
5 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and preclinical evaluation of a folic acid derivative labeled with 18F for PET imaging of folate receptor-positive tumors. J Nucl Med.
6 Chopra, A., 2-[(4-{[(2-amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(4-[18F]-fluorophenyl)carbonylamino] carbamoyl}butanoic acid. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
7 Chopra, A., 2-[(4-{[(2-amino-4-oxohydropteridin-7yl)methyl]amino}phenyl) carbonylamino]-4-{N-[(2-[18F]-fluoro(4-pyridyl))carbonylamino] carbamoyl}butanoic acid. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
8 Chopra, A., 2-[18F]Fluoropyridine-4-carbohydrazide-methotrexate (9). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Jammaz I.A., Otaibi B.A., Okarvi S., Amartey J.K. (2006). Novel synthesis of [18F]-fluorobenzene and pyridinecarbohydrazide-folates as potential PET radiopharmaceuticals. Journal of Labelled Compounds and Radiopharmaceuticals.